# N-2-(4-[^18^F]-Fluorobenzamido)ethylmaleimide coupled to cysteine-tagged epidermal growth factor

Chemical name: | N-2-(4-[^18^F]-Fluorobenzamido)ethylmaleimide coupled to cysteine-tagged epidermal growth factor
Abbreviated name: | [^18^F]FBEM-cEGF
Synonym:
Agent Category: | Peptide
Target: | Epidermal growth factor receptor
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=epidermal%20growth%20factor&cmd=DetailsSearch)]

The epidermal growth factor (EGF) receptor (EGFR) belongs to the tyrosine kinase receptor family, is activated by several different ligands such as amphiregulin, EGF, transforming growth factor α, etc., and is involved in the growth, proliferation, and differentiation of cells (1). Overexpression of the EGFR indicates a poor prognosis for patients who have solid cancerous tumors of the breast (http://cancer.gov/cancertopics/types/breast), ovaries (http://cancer.gov/cancertopics/types/ovarian), and colon (http://cancer.gov/cancertopics/types/colon-and-rectal), non-small cell cancers of the lung (http://cancer.gov/dictionary?cdrid=45323), and especially head-and-neck squamous cell carcinoma (http://www.cancer.gov/cancertopics/factsheet/Sites-Types/head-and-neck)s (HNSCC) (2). Radiolabeled antibodies (Ab) directed against specific receptors, including the EGFR, have been used for the detection (with noninvasive imaging) and therapy of the various cancers, but this approach is not entirely useful for several reasons. Due to their large size (~150 kDa), Abs show a slow uptake in the target area. In addition, the uptake is restricted to small tumors, and large lesions may not be visualized completely. Finally, Abs have a long circulating half-life and usually accumulate in the liver and the kidneys (3). Preclinical studies have shown that EGF, a natural, high-affinity ligand of the EGFR, can be labeled with radio-metals and used with positron emission tomography (PET) or single-photon emission tomography (SPECT) for the imaging of tumors that overexpress the EGFR, but these tracers may not yield optimal results because they tend to accumulate in organs located within the abdominal cavity and mask the visualization of tumors in this area of the animal body (4). Levashova et al. reported that when EGF was tagged with cysteine on the N-terminus (cEGF), radiolabeled with either ^99^Tc (for SPECT imaging) or ^64^Cu (for PET imaging), and used to visualize breast and spontaneous lung carcinoma tumors in mice, the tracer generated superior images the lesions (compared to the earlier probes) because there was low accumulation of radioactivity in the liver and kidneys (5).

Although ^18^F (half-life, ~110 min) is the most widely used radionuclide for PET imaging, no ^18^F-labeled EGF probe for the imaging of the EGFR has been reported. This is probably because the ligand lacks an amino acid that can be used to secure the ^18^F label (1). To develop an ^18^F-based EGF tracer, cEGF was conjugated to N-2-(4-[^18^F]-fluorobenzamido)ethylmaleimide ([^18^F]FBEM ), a thiol-specific ^18^F-synthon, and the biodistribution and the imaging characteristics of the radiolabeled cEGF ([^18^F]FBEM-cEGF) were investigated in mice bearing tumors generated with UM-SCC1 cells (HNSCC cells that overexpress the EGFR) (1).

### Related Resource Links

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_005228.3) of human EGFR variant 1

EGFR in OMIM (http://omim.org/entry/131550) (Online Mendelian Inheritance in Man Database)

EGFR signaling pathways (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=200086&source=NATURE&what=graphic&jpg=on) (NCI-Nature Pathways Interaction Database)

Anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-EGFR%20antibodies&cmd=DetailsSearch) in PubMed

EGFR tyrosine kinase inhibitors (http://www.ncbi.nlm.nih.gov/pubmed?term=egfr%20tyrosine%20kinase%20inhibitors&cmd=DetailsSearch) in PubMed

Chapters on anti-EGFR antibodies (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad) in MICAD

Chapters on anti-EGFRvIII antibodies (http://www.ncbi.nlm.nih.gov/books/?term=EGFRvIII%20AND%20micad%5Bbook%5D) in MICAD

Clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFRvIII+) with EGFRvIII as a target

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Synthesis%20of%20%5B18F%5DFBEM%20coupled%20to%20cEGF&cmd=DetailsSearch)]

[C4]-Monothiol cysteine-tagged human EGF was obtained from a commercial source and conjugated to [^18^F]FBEM as described by Li et al. (1). The radiochemical yield of [^18^F]FBEM-cEGF was >60%, with a radiochemical purity of >97% as determined with analytical high-performance liquid chromatography. The specific activity of the labeled peptide was reported to be 8.14 MBq/mmol (220 mCi/mmol). The in vitro stability of [^18^F]FBEM-cEGF was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=In%20vitro%20studies%20%5B18F%5DFBEM%20coupled%20to%20cEGF&cmd=DetailsSearch)]

Li et al. studied the cell binding, cell internalization, and cellular efflux of [^18^F]FBEM-cEGF in UM-SCC1 cells (obtained from the University of Michigan) (1). The cells showed a rapid binding of the label during the initial 15 min after exposure to the tracer (~3.5% of added dose); binding peaked at 3.78 ± 0.24% of the added dose by 30 min after exposure and stayed relatively constant up to 60 min after exposure. The internalization of [^18^F]FBEM-cEGF was reported to be 2.53 ± 0.23% of the added dose (73% of total binding), 2.96 ± 0.09% of the added dose (78% of total binding), and 2.79 ± 0.07% of the added dose (77% of total binding) at 15, 30, and 60 min, respectively, after exposure to the labeled peptide. Pre-incubation of the cells with excess unlabeled EGF (2 mM) reduced the binding of the label to <0.5% of the total added dose, indicating that the radiolabeled peptide had a high specificity of binding to the EGFR. When the labeled cells were incubated in serum-free medium containing no radioactivity, the cells lost 28% of the label within 15 min after initiation of the incubation (chemical form of the label in the extracellular medium was not identified) , and ~60% of the initial radioactivity was still associated with the cells after 60 min of incubation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBEM-cEGF%20Rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]FBEM-cEGF was studied in nude mice bearing UM-SCC1 cell tumors (1). The animals (under anesthesia; n = 3 mice/group) were injected through the tail vein with 3.7 MBq (100 μCi) of the tracer alone (unblocked group), or the radiolabeled compound was co-injected with 50 μg or 500 μg unlabeled EGF (blocked groups). The mice were euthanized at 30 min postinjection (p.i.) to determine the amount of radioactivity accumulated in the tumors and the various organs of interest. Results obtained from the study were presented as percent of injected dose per gram tissue (% ID/g). The uptake of label in the tumor was 1.96 ± 0.85% ID/g, 6.79 ± 1.23% ID/g, and 3.90 ± 0.36% ID/g in the unblocked group and in the groups blocked with either 50 μg and 500 μg, respectively, the maximum accumulation of radioactivity was observed in tumors of mice co-injected with 50 μg unlabeled EGF. The amount of tracer in the blood was 1.34 ± 0.28% ID/g, 3.85 ± 1.38% ID/g, and 3.56 ± 0.06% ID/g in the unblocked group and in mice blocked with either 50 μg and 500 μg, respectively, indicating that the circulation time of [^18^F]FBEM-cEGF increased in animals co-injected with the blocking doses of unlabeled EGF. The blocking doses of nonradioactive EGF increased the accumulation of radioactivity in the kidneys, lungs, and the bone, but decreased the uptake in the liver. The administration of unlabeled EGF did not change the accumulation of label in the pancreas, stomach, and the spleen.

MicroPET images were acquired from mice bearing UM-SCC1 cell tumors (n = 4 animals/time point) at 0.5, 1, and 2 h p.i. of 3.7 MBq (100 μCi) [^18^F]FBEM-cEGF (1). The tumors were clearly visible at 0.5 h p.i., and the amount of radioactivity in the lesion was determined to be 2.60 ± 0.59% ID/g, 1.87 ± 0.44% ID/g, and 0.98 ± 0.33% ID/g at 30, 60, and 120 min p.i., respectively. At 30 min p.i., the amounts of label in the kidneys and the liver were 7.23 ± 0.5% ID/g and 15.5 ± 1.21% ID/g, respectively, and by 120 min p.i. the accumulation decreased to ~2.5% ID/g and <0.5% ID/g, respectively, in these organs. The tumor/muscle ratios (calculated from the PET images) were 2.30 ± 0.51, 2.80 ± 0.47, and 4.09 ± 0.50 at 30, 60, and 120 min p.i., respectively. However, the tumor/liver ratio was very low during the initial time points, and it was reported to be 1.48 ± 0.51 at 120 min p.i.

Decay-corrected whole-body microPET images were also acquired from mice bearing UM-SCC1 cell tumors after an injection of [^18^F]FBEM-cEGF either in the presence or absence of 50 μg or 500 μg nonradioactive EGF as described above (1). From the images it was clear that, compared to the unblocked group, there was a significant increase (P < 0.01) in the uptake of tumors from animals blocked with 50 μg unlabeled EGF (2.55 ± 0.59% ID/g versus 5.99 ± 1.61% ID/g); however, tumors of animals co-injected with 500 μg unlabeled EGF had an uptake that was similar to the accumulation in tumors of the unblocked group (2.77 ± 0.78% ID/g). In addition, the liver showed a significantly lower accumulation of radioactivity (P value not reported) in the blocked animals (16.3 ± 3.08% ID/g, 7.20 ± 3.48% ID/g, and 5.22 ± 1.92% ID/g in the unblocked group and the animals co-injected with 50 μg and 500 μg unlabeled EGF mice, respectively). Compared to the unblocked mice, animals co-injected with nonradioactive EGF showed a significantly higher (P value not reported) uptake of the tracer in the kidneys. This study showed that animals injected with [^18^F]FBEM-cEGF alone showed a high accumulation of the tracer in the liver, which was attributed to high expression of the EGFR in this organ (1), but the tumors showed a low amount of label. However, when [^18^F]FBEM-cEGF was co-injected withf unlabeled EGF, the amount of radioactivity in the liver decreased and the tumors showed an increase in accumulation of the probe.

From these studies, the investigators concluded that [^18^F]FBEM-cEGF can be used in rodents for the noninvasive visualization of tumors that overexpress the EGFR, provided that the blocking of the liver with unlabeled EGF is optimized (1). In addition, this probe can probably be used for the quantification of EGFR activity in the tumors of these animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBEM-cEGF%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FBEM-cEGF%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22109665&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies reported in this chapter were supported in part by the Intramural Research Program of the National Institute of Biomedical Imaging and Bioengineering (NIBIB), National Institutes of Health (NIH).

## References

1 Li W., Niu G., Lang L., Guo N., Ma Y., Kiesewetter D.O., Backer J.M., Shen B., Chen X. (2012). PET imaging of EGF receptors using [(18)F]FBEM-EGF in a head and neck squamous cell carcinoma model. Eur J Nucl Med Mol Imaging.
2 Beckford Vera D.R., Eigner S., Henke K.E., Lebeda O., Melichar F., Beran M. (2012). Preparation and preclinical evaluation of (177)Lu-nimotuzumab targeting epidermal growth factor receptor overexpressing tumors. Nucl Med Biol.
3 Sharkey R.M., Goldenberg D.M. (2011). Cancer radioimmunotherapy. Immunotherapy.
4 Velikyan I., Sundberg A.L., Lindhe O., Hoglund A.U., Eriksson O., Werner E., Carlsson J., Bergstrom M., Langstrom B., Tolmachev V. (2005). Preparation and evaluation of (68)Ga-DOTA-hEGF for visualization of EGFR expression in malignant tumors. J Nucl Med.
5 Levashova Z., Backer M.V., Horng G., Felsher D., Backer J.M., Blankenberg F.G. (2009). SPECT and PET imaging of EGF receptors with site-specifically labeled EGF and dimeric EGF. Bioconjug Chem.